# ^68^Ga-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-1,2-diaminoethane-γ-folate (P3246)

Chemical name: | ^68^Ga-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-1,2-diaminoethane-γ-folate (P3246)
Abbreviated name: | ^68^Ga-P3246
Synonym: | ^68^Ga-NODAGA-folate
Agent category: | Compound
Target: | Folate receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3246)]

Folic acid (folate) is a water-soluble B vitamin (1) that is essential for methylation and DNA synthesis. The primary pathway for entry of folate into cells is through the facilitated transporter, which has a low affinity for folate (Michaelis constant (K_m_) = 1–5 μM). Some cells in the choroid plexus, kidney, lung, thyroid, spleen, placenta, and thymus also possess a higher-affinity receptor (dissociation constant (K_d_) = 0.5 nM) that allows folate uptake via receptor-mediated endocytosis. Some human epithelial tumor cells have been found to overexpress folate receptors (2). More than 90% of human ovarian and endometrial cancers express the high-affinity folate receptor, which is absent in the corresponding normal tissues. Breast, colorectal, renal, and lung carcinomas also overexpress the high-affinity folate receptor but at lower frequencies (20%–50%). Activated macrophages, but not resting macrophages, have also been found to have the high-affinity folate receptor (3).

Several folate-based conjugates (^111^In-DTPA-folate, ^99m^Tc-EC-folate, and [^18^F]FBA-folate) have been studied in tumor imaging (4-8). Deferoxamine (DF), a chelating agent, was conjugated to folic acid to form a mixture of two isomers, DF-α-folate and DF-γ-folate. Only the DF-γ-folate isomer was able to displace [^3^H]folic acid from its receptors, with a 50% inhibition concentration similar to that of folic acid (2.5 nM versus 2.4 nM) (9). Fani et al. (10) prepared a γ-folate conjugate with tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) and 1,2-diaminoethane as a spacer to form P3026 (http://www.ncbi.nlm.nih.gov/books/NBK55064/), which was labeled with ^68^Ga for positron emission tomography (PET) imaging of folate receptors in tumors. To further the quest for a ^68^Ga-folate conjugate for clinical application, folic acid was conjugated to 1,4,7-triazacyclononane,1-glutaric acid-4,7-acetic acid (NODAGA) via 1,2-diaminoethane as a linker between the NODAGA and folic acid (P3246) (11). ^68^Ga-P3246 was evaluated as a PET agent for imaging folate receptor expression in a mouse tumor model. ^67/68^Ga-P3246 exhibited a higher tumor/blood ratio than ^67/68^Ga-P3026 in the same tumor model.

### Related Resource Links:

- Chapters in MICAD (folate receptor (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=folate+receptor+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (folate receptor (http://www.ncbi.nlm.nih.gov/gene/2348))
- Articles in OMIM (folate receptor (http://www.ncbi.nlm.nih.gov/omim/136430))
- Clinical trials (folate receptors (http://www.clinicaltrials.gov/ct2/results?term=folate+receptor))
- Drug information in FDA (folate receptor (http://google2.fda.gov/search?q=folate+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3246%20and%20synthesis)]

Fani et al. (11) coupled P3246 (12 nmol) with ^68^Ga in sodium acetate buffer (pH 4.0) for 10 min at 25°C to yield ^68^Ga-P3246 with >92% radiochemical purity. Radiochemical yields exceeded 95% with a specific activity of ~30 MBq/nmol (0.81 mCi/nmol). ^67^Ga-P3246 was similarly radiolabeled with a specific activity of ~3 MBq/nmol (0.081 mCi/nmol). ^68^Ga-P3238 was prepared with similar specific activity as ^68^Ga-P3246.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3246%20and%20in%20vitro)]

The human nasopharyngeal carcinoma KB cell line folate receptors were studied with ^67^Ga-P3246 saturation binding studies at 4°C (11). ^67^Ga-P3246 showed a K_d_ (affinity constant) of 5.61 ± 0.96 nM, which was similar to the K_d_ value (4.65 ± 0.82 nM) for ^67^Ga-P3026 (the DOTA-folate conjugate). ^67^Ga-P3246 (2.5 nM) was rapidly associated (bound to the cell surface and internalized) with KB cells at 37°C, with 60% of incubation dose (ID) at 30 min and 72% ID at 4 h. Approximately 15% ID ^67^Ga-P3246 was internalized at 4 h. Excess folate blocked the cell-associated radioactivity to <1% ID. Approximately 76% of radioactivity was retained in the cells after 4 h incubation in fresh medium.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3246%20and%20rodentia)]

Fani et al. (11) performed ex vivo biodistribution studies of 0.4 nmol ^67/68^Ga-P3246 in nude mice (n = 3–5/group) bearing KB tumor xenografts. Accumulation of ^67/68^Ga-P3246 in the KB tumors was 15.56 ± 3.67, 18.42 ± 0.74, 16.29 ± 4.46, and 14.32 ± 5.80% injected dose/gram (ID/g) at 1, 2, 4, and 24 h after injection, respectively. The organ with the highest accumulation at 4 h after injection was the kidney (130% ID/g), followed by the salivary gland (8.6% ID/g), pancreas (2.9% ID/g), adrenal (2.8% ID/g), heart (2.0% ID/g), muscle (1.8% ID/g), stomach (1.5% ID/g), and liver (1.1% ID/g). The accumulation in the blood was low (0.06% ID/g) at 4 h. The tumor/blood ratios were 81, 207, 254, and 391 at 1, 2, 4, and 24 h, respectively. Pretreatment with excess folate (40 nmol, 5 min before ^67/68^Ga-P3246 injection) reduced the radioactivity accumulation by >85% in the folate receptor-positive tumor, salivary glands, and kidneys at 4 h after injection. Pretreatment with pemetrexed (60 min before ^67^Ga-P3246 injection), a folate analog metabolic inhibitor, significantly reduced the kidney accumulation of ^67/68^Ga-P3246 by >70% at 1 h and 4 h after injection. On the other hand, little inhibition by pemetrexed was observed in the tumor and other organs. ^67/68^Ga-P3246 exhibited higher tumor/blood ratios than its ^67/68^Ga-DOTA counterpart (^67/68^Ga-P3026 with tumor/blood ratios of 36 at 1 h, 50 at 2 h, and 70 at 4 h).

Whole-body PET imaging scans were performed for 60 min after injection of 10 MBq (0.27 mCi) ^68^Ga-P3246 (0.4 nmol) in nude mice bearing KB tumor xenografts (the number of mice used was not reported) (11). The highest radioactivity levels were visualized in the KB tumor, salivary glands, and kidneys, with standard uptake values of 2.2, 1.8, and 10 at 60 min, respectively. The accumulation of ^68^Ga-P3246 in the kidneys was blocked by pre-injection of pemetrexed, whereas the accumulation in the tumor and salivary glands remained at the same levels. No blocking studies using excess folate were reported for the PET studies.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3246%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3246%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3246%20and%20human)]

No publication is currently available.

## References

1 Stanger O. (2002). Physiology of folic acid in health and disease. Curr Drug Metab.
2 Ke C.Y., Mathias C.J., Green M.A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
3 Nakashima-Matsushita N., Homma T., Yu S., Matsuda T., Sunahara N., Nakamura T., Tsukano M., Ratnam M., Matsuyama T. (1999). Selective expression of folate receptor beta and its possible role in methotrexate transport in synovial macrophages from patients with rheumatoid arthritis. Arthritis Rheum.
4 Mathias C.J., Hubers D., Low P.S., Green M.A. (2000). Synthesis of [(99m)Tc]DTPA-folate and its evaluation as a folate-receptor-targeted radiopharmaceutical. Bioconjug Chem.
5 Mathias C.J., Lewis M.R., Reichert D.E., Laforest R., Sharp T.L., Lewis J.S., Yang Z.F., Waters D.J., Snyder P.W., Low P.S., Welch M.J., Green M.A. (2003). Preparation of 66Ga- and 68Ga-labeled Ga(III)-deferoxamine-folate as potential folate-receptor-targeted PET radiopharmaceuticals. Nucl Med Biol.
6 Mathias C.J., Wang S., Low P.S., Waters D.J., Green M.A. (1999). Receptor-mediated targeting of 67Ga-deferoxamine-folate to folate-receptor-positive human KB tumor xenografts. Nucl Med Biol.
7 Mathias C.J., Wang S., Waters D.J., Turek J.J., Low P.S., Green M.A. (1998). Indium-111-DTPA-folate as a potential folate-receptor-targeted radiopharmaceutical. J Nucl Med.
8 Bettio A., Honer M., Muller C., Bruhlmeier M., Muller U., Schibli R., Groehn V., Schubiger A.P., Ametamey S.M. (2006). Synthesis and Preclinical Evaluation of a Folic Acid Derivative Labeled with 18F for PET Imaging of Folate Receptor-Positive Tumors. J Nucl Med.
9 Wang S., Lee R.J., Mathias C.J., Green M.A., Low P.S. (1996). Synthesis, purification, and tumor cell uptake of 67Ga-deferoxamine--folate, a potential radiopharmaceutical for tumor imaging. Bioconjug Chem.
10 Fani M., Wang X., Nicolas G., Medina C., Raynal I., Port M., Maecke H.R. (2011). Development of new folate-based PET radiotracers: preclinical evaluation of Ga-DOTA-folate conjugates. Eur J Nucl Med Mol Imaging.
11 Fani M., Tamma M.L., Nicolas G.P., Lasri E., Medina C., Raynal I., Port M., Weber W.A., Maecke H.R. (2012). In Vivo Imaging of Folate Receptor Positive Tumor Xenografts Using Novel (68)Ga-NODAGA-Folate Conjugates. Mol Pharm.